# Aqueous colloidal nanoemulsion of perfluorocarbon polymers

Chemical name: | Aqueous colloidal nanoemulsion of perfluorocarbon polymers
Abbreviated name: | CS-1000
Synonym:
Agent Category: | Nanoparticles
Target: | Cells
Target Category: | Others (cell tracking)
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | ^19^F
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=19F%20MRI)]

Cell tracking with magnetic resonance imaging (MRI) is achieved by labeling cells of interest with a contrast agent or by transducing cells to express reporter genes (1, 2). In both preclinical and clinical situations, iron oxide–based agents are typically used and provide a strong change in signal per unit of metal in T2-weighted images without significant effect on labeled cells and on the host. However, MRI quantification of iron oxide concentration is still not reliable because there is no clear correlation between the iron oxide signal and the number of labeled cells and measuring a decrease in signal has always been a problem (2, 3).

An alternative development for quantitative cell tracking is the application of ^19^F in MRI imaging (4, 5). Endogenous fluorine is found primarily in bones and teeth as solid fluorides, and it has a very short T2 relaxation time and results in an undetectable signal with ^19^F MRI. Cell tracking studies with fluorinated tracers have shown that the labeled cells can be detected on the order of 10^4^–10^5^ cells per voxel for clinical MRI systems and 10^3^–10^4^ cells per voxel for high-field animal scanners (3, 6). The MRI images positive for the ^19^F signal are extremely selective for the labeled cells. The absolute number of the labeled cells could be measured directly from the in vivo^19^F images, thus providing a quantitative biomarker. The positive ^19^F signal is also of great advantage for cell tracking in regions such as lungs, tissues and organs of the abdominal cavity, and bones. Although cell division and subsequent dilution of the tracers limit long-term cell tracking and decrease the accuracy of cell quantification, it has been shown that the absolute cell number can be quantified for up to 3 weeks in actively dividing cells in mice and that the underestimation of the cell number is within tolerable limits (usually two- to four-fold lower depending on the cell division rate and length of time) (6). This error range can be reduced if the cell division rate is known. Similar to what has been observed with iron oxide agents, the death of the labeled cells may result in transfer of the tracers to phagocytes, resulting in false positive signals (3, 7). CS-1000 is a commercially available reagent specifically formulated to facilitate its internalization into various cell types ex vivo regardless of the cell's inherent phagocytic ability (3, 7). CS-1000 is an aqueous colloidal nanoemulsion of perfluorocarbon polymers. Perfluorocarbon is both hydrophobic and lipophobic, and it does not become associated with cell membranes (3, 8). The perfluorocarbon component maintains its structure at typical lysosomal pH values and is not degraded by cell enzymes found in the body, which allows it to provide long-lasting intracellular labeling. Bonetto et al. investigated the utility of CS-1000 for tracking and quantification of human dendritic cells (DCs) directly from image data (3). The investigators showed that the minimum number of labeled cells detectable at 7 T was ~2,000 per voxel, with 1.7 × 10^13^ fluorine atoms per cell (3). DCs are antigen-presenting cells of the immune system with key roles in inducing immunity, which forms the rationale of DC immunotherapy (5). Monocyte-derived DCs do not divide (3), which makes DC quantification and tracking studies particularly suitable because there is no signal reduction and data misinterpretation is less likely because the results are not affected by the uncontrolled process of cell division.

### Related Resource Links:

- Chapters on ^19^F MRI in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=19F%20AND%20micad%5bbook%5d)
- Chapters on MRI cell tracking in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=cell%20tracking%20AND%20micad%5bbook%5d)
- Drug information of CS-1000 (http://www.celsense.com/cellsense_whitepaper.pdf)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20839261)]

CS-1000 is commercially available. The total fluorine content is 100 mg/ml, and the droplet size of the nanoemulsion is ~180 nm (3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20839261)]

Bonetto et al. analyzed the cell labeling efficiency with DCs and CS-1000 (3). DCs were generated from mononuclear peripheral blood cells from donor blood. CS-1000 (50–200 µl/million cells) was added to immature DCs on day 3 of culture, and the cells were incubated for 3 days before the addition of maturation factors. DCs took up CS-1000 effectively, without a need for transfection aids. Cellular uptake appeared to be saturated at 140 µl (fluorine content, 100 mg/ml) CS-1000 per million cells. Significant toxicity was observed only at high concentrations (a threshold value was not provided) of CS-1000. Labeling with 75 µl CS-1000 per million cells was used by investigators for their experiments. This yielded 1.7 ± 0.1 × 10^1319^F atoms/cell with an acceptable cell viability of 80 ± 6%. Cell labeling was homogeneous on the basis of the ^19^F content/cell among independent samples. CS-1000 had no evident side effects on DC viability, antigen expression, or maturation at the concentration of 75 µl CS-1000 per million cells.

Detection sensitivity was evaluated with a 7 T MRI system, and a comparison was performed among CS-1000, ProHance (a gadolinium (Gd)-based agent, 1 mM/5 x 10^5^ cells) and Ferumoxide (a superparamagnetic iron oxide (SPIO)-based agent, 200 µg/5 x 10^5^ cells) (3). Labeled cells were suspended in gelatin. The minimum detectable density of ^19^F-labeled cells was comparable to that of Gd-labeled cells at <2,000 cells/voxel when assessed visually. The detection limit with SPIO was lower at ~125 cells/voxel. However, the detection sensitivity is related to the amounts of F-19, Gd, and Fe used for cell labeling.

The cell number was determined after cells were labeled with Gd, SPIO, or ^19^F and suspended at various densities in gelatin (3). A linear relationship between the ^19^F intensity and the number of cells per voxel was observed. A similar linear relationship existed between the signal/noise ratio and the cell density. Thus, the cell number can be calculated directly from the image data if the label content per cell is known. For the Gd- and SPIO-labeled cells, complex relationships were observed between T1 and T2* relaxation times and the relative contrast in the images. The change in contrast began to saturate at ~8,000 cells/voxel with Gd and as early as 800 cells/voxel with SPIO. These issues complicated the cell number quantification with Gd- and SPIO-based contrast agents but not with ^19^F labels.

The detection sensitivity over tissue background was evaluated after injection of the labeled DCs (1.5 million) as a bolus into isolated bovine muscle. The unlabeled cells showed a typical nonhomogeneous background from the biological tissue. The contrast due to SPIO was apparent, and the SPIO-labeled cells displayed a sharp decrease in the signal intensity. The Gd-labeled cells were not readily detected in this image over the background. The ^19^F-labeled cells were clearly visible and were readily identified and differentiated against the ^1^H tissue underlay. The detection sensitivity was on the order of 2,000 cells/voxel, confirming that the sensitivity and quality of ^19^F images are not affected by the presence of tissue background (3).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20839261)]

The feasibility of in vivo^19^F cell tracking was tested after ~3 × 10^6^ mature, labeled, human DCs were injected subcutaneously into the quadriceps muscle of a female NOD-SCID mouse. Labeled cells were clearly visible in the ^19^F image, and at 12 h after injection cells were observed to be localized in a region anatomically consistent with the proximal draining inguinal lymph node, indicating cell migration away from the injection site.

In summary, the detection limit with CS-1000 was 2,000 cells/voxel at 7 T with 1.7 ± 0.1 × 10^1319^F atoms/cell, which translates to a detection limit of ~9,000 cells/voxel at 3 T. A typical DC vaccination study utilizes an intranodal or intradermal injection of ~10 million cells, with 30,000–200,000 cells migrating to secondary lymph nodes as detected with scintigraphy on ^111^In-labeled DCs (9). Detection of 30,000 cells in vivo at 3 T with a reasonable signal/noise ratio for ^19^F images would require <30 min with a conventional fast spin-echo sequence, as calculated by Bonetto at al (3). This is well within acceptable limits for clinical studies. Bonetto et al. concluded that ^19^F MRI for quantitative cell tracking in a clinical setting has great potential (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Arbab A.S., Liu W., Frank J.A. (2006). Cellular magnetic resonance imaging: current status and future prospects. Expert Rev Med Devices.
2 Bulte J.W. (2009). In vivo MRI cell tracking: clinical studies. AJR Am J Roentgenol.
3 Bonetto, F., M. Srinivas, A. Heerschap, R. Mailliard, E.T. Ahrens, C.G. Figdor, and I.J. de Vries, A novel (19)F agent for detection and quantification of human dendritic cells using magnetic resonance imaging. Int J Cancer, 2010
4 Chen J., Lanza G.M., Wickline S.A. (2010). Quantitative magnetic resonance fluorine imaging: today and tomorrow. Wiley Interdiscip Rev Nanomed Nanobiotechnol.
5 Srinivas M., Aarntzen E.H., Bulte J.W., Oyen W.J., Heerschap A., de Vries I.J., Figdor C.G. (2010). Imaging of cellular therapies. Adv Drug Deliv Rev.
6 Srinivas M., Turner M.S., Janjic J.M., Morel P.A., Laidlaw D.H., Ahrens E.T. (2009). In vivo cytometry of antigen-specific t cells using 19F MRI. Magn Reson Med.
7 Helfer B.M., Balducci A., Nelson A.D., Janjic J.M., Gil R.R., Kalinski P., de Vries I.J., Ahrens E.T., Mailliard R.B. (2010). Functional assessment of human dendritic cells labeled for in vivo (19)F magnetic resonance imaging cell tracking. Cytotherapy.
8 Lanza G.M., Winter P.M., Neubauer A.M., Caruthers S.D., Hockett F.D., Wickline S.A. (2005). 1H/19F magnetic resonance molecular imaging with perfluorocarbon nanoparticles. Curr Top Dev Biol.
9 De Vries I.J., Krooshoop D.J., Scharenborg N.M., Lesterhuis W.J., Diepstra J.H., Van Muijen G.N., Strijk S.P., Ruers T.J., Boerman O.C., Oyen W.J., Adema G.J., Punt C.J., Figdor C.G. (2003). Effective migration of antigen-pulsed dendritic cells to lymph nodes in melanoma patients is determined by their maturation state. Cancer Res.